# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Ser-rich Cys knot scaffold grafted with integrin α_v_β_6_-binding peptide RSLARTDLDHLRGR

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Ser-rich Cys knot scaffolds grafted with integrin α_v_β_6_-binding peptide RSLARTDLDHLRGR
Abbreviated name: | ^64^Cu-DOTA-S_0_2
Synonym:
Backbone: | Peptide
Target: | Integrin α_v_β_6_
Mechanism: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_ and α_v_β_6_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Integrin α_v_β_6_ plays an important role in the development of epithelial cells and is nearly undetectable on adult normal tissues. However, the levels of α_v_β_6_ integrin can be upregulated during tissue remodeling and wound healing (11). On the other hand, α_v_β_6_ integrin is strongly expressed on tumor cells of the oral cavity, pancreas, breast, ovary, colon, and stomach (12-14). α_v_β_6_ integrin affects tumor growth, tumor invasiveness, and metastasis (13). α_v_β_6_ binds to the RGD motif in fibronectin, tenascin, and the viral protein 1 (VP1) of foot-and-mouth disease virus (FMDV) (15). FMDV binds to cells through the RGD motif of the GH loop of the VP1. A consensus α_v_β_6_-binding motif DLXXL was identified by using phage display screening with minimal binding to α_v_β_3_, α_IIb_β_3_, and α_v_β_5_ (16). Engineered cysteine knot peptides (knots) comprise a rigid molecular scaffold of ~4 kDa with three disulfide bonds and a centrally located β sheet. Kimura et al. (17) grafted a α_v_β_6_-binding peptide (RSLARTDLDHLRGR) into the loop 1 of a Ser-rich knot to produce the knot known as S_0_2, which was radiolabeled with ^64^Cu via 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugation to form ^64^Cu-DOTA-S_0_2 as a positron emission tomography (PET) probe for in vivo imaging of α_v_β_6_ integrin in tumor-bearing nude mice.

### Related Resource Links:

- Chapters in MICAD (knot peptide (http://www.ncbi.nlm.nih.gov/books?term=knot%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_6_ integrin (http://www.ncbi.nlm.nih.gov/gene/3694))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_6_ integrin (http://www.ncbi.nlm.nih.gov/omim/147558))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20synthesis)]

Kimura et al. (17) reported the synthesis of ^64^Cu-DOTA-R_0_2. S_0_2 was synthesized and folded. The N-terminus amine of S_0_2 was conjugated with DOTA-N-hydroxysuccinimide ester for labeling with ^64^Cu. The radiochemical purity was >95%, with a specific activity of 18.5 MBq/nmol (0.5 mCi/nmol) at the end of purification. The labeling yield was >80%. Molecular masses of S_0_2 (3.877 kDa) and DOTA-S_0_2 (4.258 kDa) were confirmed with matrix-assisted laser desorption/ionization-mass spectrometry. ^64^Cu-DOTA-S_0_2 remained >95% intact in mouse serum for 24 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28in%20vitro%20or%20cell%29)]

Competitive binding of soluble integrins α_v_β_6_, α_v_β_3_, α_v_β_5_, and α_5_β_1_ to yeast cells expressing S_0_2 was determined with flow cytometry (17). The binding affinity (K_d_) value for α_v_β_6_ was 6.0 ± 0.1 nM. Integrins α_v_β_3_, α_v_β_5_, and α_5_β_1_ (10–300 nM) exhibited little binding to S_0_2. Cellular accumulation of ^64^Cu-DOTA-S_0_2 was determined in A431 human epidermoid cancer and BxPC3 human pancreatic cancer cells (high α_v_β_6_ expression), and HEK293 human embryonic kidney cells (low α_v_β_6_ expression). A431 and BxPC3 cells exhibited ~50% higher cellular radioactivity than that of HEK293 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20rodentia)]

Kimura et al. (17) performed biodistribution studies with 3.7 MBq (0.1 mCi, 0.15 nmol) ^64^Cu-DOTA-S_0_2 in nude mice (n = 3/group) bearing BxPC3 xenografts. Data were obtained at 1 h and 24 h after injection. ^64^Cu-DOTA-S_0_2 had blood levels of 0.29% and 0.23% injected dose (ID)/g at 1 h and 24 h. The initial tracer accumulation in the α_v_β_6_-integrin-expressing BxPC3 tumors was about 1.80% ID/g at 1 h and decreased to 1.48% ID/g at 24 h. At 60 min, the highest radioactive concentration was found in the kidney (26.5% ID/g), followed by the liver (3.03% ID/g), intestine (1.28% ID/g), lung (1.03% ID/g), and stomach (0.79% ID/g). The spleen, bone, muscle, skin, pancreas, and heart showed low levels of radioactivity (<0.3% ID/g). The kidney accumulation of ^64^Cu-DOTA-S_0_2 was two- to three-fold lower than the kidney accumulation of ^64^Cu-DOTA-R_0_2 and ^64^Cu-DOTA-R_0_1 (arginine-rich knots). The tumor/muscle ratios for ^64^Cu-DOTA-S_0_2 were 6.22 and 6.36 at 1 h and 24 h, respectively. No blocking studies were performed.

^64^Cu-DOTA-S_0_2 PET imaging studies were performed in nude mice (n = 3) bearing both BxPC3 and HEK293 xenografts at 1, 2, 4, and 24 h after injection of 3.7 MBq (0.1 mCi, 0.15 nmol) ^64^Cu-DOTA-S_0_2 (17). The BxPC3 tumors were clearly visualized as early as 1 h and as late as 24 h after injection. Major radioactivity was observed in the urinary bladder and kidneys. Region-of-interest analysis showed the tumor accumulation of ^64^Cu-DOTA-S_0_2 was ~2% ID/g in BxPC3 tumors compared with 0.5% ID/g in HEK293 tumors. Average tumor/background ratios were ~10 (BxPC3) and ~2 (HEK293). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=arginine%20knot%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Breuss J.M., Gallo J., DeLisser H.M., Klimanskaya I.V., Folkesson H.G., Pittet J.F., Nishimura S.L., Aldape K., Landers D.V., Carpenter W., et al. (1995). Expression of the beta 6 integrin subunit in development, neoplasia and tissue repair suggests a role in epithelial remodeling. J Cell Sci.
12 Thomas G.J., Nystrom M.L., Marshall J.F. (2006). Alphavbeta6 integrin in wound healing and cancer of the oral cavity. J Oral Pathol Med.
13 Kawashima A., Tsugawa S., Boku A., Kobayashi M., Minamoto T., Nakanishi I., Oda Y. (2003). Expression of alphav integrin family in gastric carcinomas: increased alphavbeta6 is associated with lymph node metastasis. Pathol Res Pract.
14 Bates R.C. (2005). The alphaVbeta6 integrin as a novel molecular target for colorectal cancer. Future Oncol.
15 DiCara D., Rapisarda C., Sutcliffe J.L., Violette S.M., Weinreb P.H., Hart I.R., Howard M.J., Marshall J.F. (2007). Structure-function analysis of Arg-Gly-Asp helix motifs in alpha v beta 6 integrin ligands. J Biol Chem.
16 Kraft S., Diefenbach B., Mehta R., Jonczyk A., Luckenbach G.A., Goodman S.L. (1999). Definition of an unexpected ligand recognition motif for alphav beta6 integrin. J Biol Chem.
17 Kimura R.H., Teed R., Hackel B.J., Pysz M.A., Chuang C.Z., Sathirachinda A., Willmann J.K., Gambhir S.S. (2012). Pharmacokinetically stabilized cystine knot peptides that bind alpha-v-beta-6 integrin with single-digit nanomolar affinities for detection of pancreatic cancer. Clin Cancer Res.